# ^111^In-Diethylenetriamine pentaacetic acid-pertuzumab

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-pertuzumab
Abbreviated name: | ^111^In-DTPA-pertuzumab
Synonym:
Agent category: | Antibody
Target: | Epidermal growth factor (EGF) receptor, HER2
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In)]

Epidermal growth factor (EGF) is a cytokine composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains each: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab) for anti-cancer therapies in both Europe and North America. Labeled trastuzumab (^111^In-trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_) has been developed for HER2 imaging in human breast cancer (12-16). Resistance to trastuzumab therapy may be a result of its induction of HER2 receptor downmodulation (17). Pertuzumab is a new class of humanized mAb against HER2 that binds to a different epitope than trastuzumab does. On binding to the HER2 receptor, pertuzumab inhibits the receptor dimerization and the downstream signal transduction pathway. It is being evaluated in several clinical trials (http://clinicaltrials.gov/ct2/results?term=pertuzumab) to treat a variety of cancers. McLarty et al. (18) has performed single-photon emission computed tomography (SPECT) studies using ^111^In-diethylenetriamine pentaacetic acid-pertuzumab (^111^In-DTPA-pertuzumab) to investigate trastuzumab-mediated HER2 downregulation in human breast cancer xenografts in nude mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1956)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=HER2)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), Pertuzumab (http://www.clinicaltrials.gov/ct2/results?term=Pertuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In+synthesis)]

DTPA dianhydride (2.7 mM) and pertuzumab (4:1 molar ratio) were incubated in sodium bicarbonate buffer (pH 8) for 1 h at room temperature (18). DTPA Pertuzumab was purified with ultrafiltration. There were 1.4 DTPA molecules per antibody. DTPA Pertuzumab was mixed with a predetermined amount of ^111^In, and the mixture was incubated for 1 h at room temperature. ^111^In-DTPA-pertuzumab was purified with G-50 column chromatography with a radiochemical purity of >97. The radiochemical yield and the specific activity of ^111^In-DTPA-pertuzumab were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In%20and%20in%20vitro)]

In vitro binding specificity tests showed that binding of ^111^In-DTPA-pertuzumab (500 pM) to SKBr-3 cells expressing HER2 was mediated by the receptors because saturation of receptors by incubation with non-labeled pertuzumab significantly decreased binding of ^111^In-DTPA-pertuzumab (18). ^111^In-DTPA-pertuzumab exhibited a K_d_ value of 2.0 ± 1.0 nM and a B_max_ of 1.2 ± 0.2 × 10^6^ receptor sites per cell. On the other hand, the binding of ^111^In-DTPA-pertuzumab to SKBr-3 cells was not displacedby up to 1,000 nM trastuzumab. The saturation binding of ^111^In-DTPA-pertuzumab to SKBr-3 cells exposed to trastuzumab (0.1 nM) was reduced by 18%, 30%, and 38% at 24, 48, and 72 h, respectively, after pretreatment with trastuzumab at 37°C. The saturation binding of ^111^In-DTPA-pertuzumab to MDA-MB-361 cells (moderate HER2 expression) exposed to trastuzumab (0.1 nM) was reduced by 69%, 68%, and 68% at 24, 48, and 72 h, respectively, after pretreatment with trastuzumab at 37°C. The differences between SKBr-3 and MDA-MB-362 in trastuzumab-induced HER2 downregulation may be because of faster internalization of ^111^In-DTPA-pertuzumab in MDA-MB-362 cells than SKBr-3. Incubation with rituximab (anti-CD20) and control IgG had no effect on the binding of ^111^In-DTPA-pertuzumab to these cells compared with untreated cells. Confocal microscopy and confocal cytometry confirmed the reduction of HER2 density on the cells pretreated with trastuzumab, indicating the downregulation of HER2 induced by trastuzumab.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In%20and%20rodentia)]

McLarty et al. (18) performed ex vivo biodistribution studies of ^111^In-DTPA-pertuzumab (0.066 nmol) in nude mice (n = 3–4/group) bearing MDA-MB-361 xenografts at 72 h after intravenous injection. The tracer accumulation in the tumors was 34.6% injected dose per gram (ID/g). The normal organ with the highest radioactivity was the kidney (15.3% ID/g), followed by the liver (8.5% ID/g), spleen (7.8% ID/g), blood (5.9% ID/g), and intestines (1.5–2.0% ID/g). Tumor/blood and tumor/muscle ratios were 5.9 and 37.9, respectively. Pretreatment with pertuzumab (6.6 nmol) 24 h before ^111^In-DTPA-pertuzumab injection blocked the tumor radioactivity by 78% at 72 h after injection. Tumor accumulation of ^111^In-DTPA-pertuzumab was reduced by 53% and 78% with 3 d pretreatment with trastuzumab (26 nmol/kg) and with a single dose of 26 nmol/kg followed by two 13 nmol/kg weekly doses (52 nmol/kg total), respectively. Pretreatment with rituximab (anti-CD20) and control IgG had little effect on the tumor accumulation of ^111^In-DTPA-pertuzumab. SPECT gamma imaging analysis was performed in nude mice bearing MDA-MB-361 tumors at 72 h after injection of ^111^In-DTPA-pertuzumab. The tumors were clearly visualized, whereas pretreatment with trastuzumab (3 d) reduced tumor radioactivity two-fold because of downregulation of HER2 by trastuzumab. The three-dose pretreatment with trastuzumab for 3 weeks almost completely blocked accumulation in the tumors because of an almost complete elimination of HER2-positive tumor cells as determined with immunohistochemical staining.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pertuzumab+111In%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Albanell J., Codony J., Rovira A., Mellado B., Gascon P. (2003). Mechanism of action of anti-HER2 monoclonal antibodies: scientific update on trastuzumab and 2C4. Adv Exp Med Biol.
18 McLarty K., Cornelissen B., Cai Z., Scollard D.A., Costantini D.L., Done S.J., Reilly R.M. (2009). Micro-SPECT/CT with 111In-DTPA-pertuzumab sensitively detects trastuzumab-mediated HER2 downregulation and tumor response in athymic mice bearing MDA-MB-361 human breast cancer xenografts. J Nucl Med.